# N,N-Diethyl-2-(2-(3-[^125^I]iodo-4-methyoxyphenyl)-5,7-dimethyl-pyrazolo(1,5-a)pyrimidin-3-yl)-acetamide

Chemical name: | N,N-Diethyl-2-(2-(3-[^125^I]iodo-4-methyoxyphenyl)-5,7-dimethyl-pyrazolo(1,5-a)pyrimidin-3-yl)-acetamide
Abbreviated name: | [^125^I]IodoDPA-713
Synonym:
Agent category: | Compound
Target: | Peripheral-type benzodiazepine receptor (PBR), also known as translocator protein (TSPO)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT)
Source of signal: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iodoDPA-713)]

Benzodiazepines are potent psychoactive drugs used for their sedative and anxiolytic properties (1, 2). There are two types of benzodiazepine receptors, which have been designated as the central benzodiazepine receptor (CBR) and the peripheral benzodiazepine receptor (PBR). PBR is also known as the translocator protein (TSPO). CBR is found exclusively in the central nervous system on the membranes of neurons and is coupled with the γ-aminobutyric acid receptor/chloride channel (3). In contrast, PBR is a mitochondrial protein found in brain and peripheral tissues (adrenal gland, heart, lung, kidney, and testis) (4). The brain has lower levels of PBR than do peripheral tissues, while both glial cells and macrophages contain high levels of PBR (5-7). Increased PBR expression after brain injury or neuroinflammation is associated with microglial activation, such as occurs with the neuronal damage that accompanies several neurodegenerative diseases, including Alzheimer’s disease, Wernicke’s encephalopathy, multiple sclerosis, and epilepsy.

PBR has been studied in vivo with positron emission tomography (PET) using 1-(2-chlorophenyl)-N-[^11^C]methyl-N-(1-methylpropyl)-3-isoquinoline carboxamide ([^11^C]PK11195), an isoquinoline carboxamide with specific PBR antagonistic activity. [^11^C]PK11195 has been developed as a PET agent for non-invasive studies of microglia and macrophage activation in the brain, lung, and heart. However, accumulation of this tracer in the brain is limited with a poor signal/noise ratio. Other ligands displaying better brain kinetics have recently been synthesized and studied. Among them, N,N-diethyl-2-(2-(4-[^11^C]methoxyphenyl)-5,7-dimethyl-pyrazolo(1,5-a)pyrimidin-3-yl)-acetamide ([^11^C]DPA-713), a compound from the family of pyrazolopyrimidines (8), has shown a slightly higher affinity (K_i_ = 4.7 nM) for PBR than does [^11^C]PK11195 (K_i_ = 9.3 nM). N,N-Diethyl-2-(2-(3-[^125^I]iodo-4-methyoxyphenyl)-5,7-dimethyl-pyrazolo(1,5-a)pyrimidin-3-yl)-acetamide ([^125^I]iodoDPA-713), a DPA-713 analog, has been developed for single-photon emission computed tomography (SPECT) imaging of PBR in the brain (9).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=PBR%5BAll+Fields%5D+AND+micad%5Bbook%5D)
- Gene information in NCBI (PBR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=706%5Buid%5D))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=109610)
- Clinical trials (PBR (http://www.clinicaltrials.gov/ct2/results?term=pk11195+OR+PBR))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iodoDPA-713%20and%20synthesis)]

Wang et al. (9) reported the synthesis of [^125^I]iodoDPA-713. To a solution of N,N-diethyl-2-(2-(4-hydroxy-phenyl)-5,7-dimethyl-pyrazolo(1,5-a)pyrimidin-3-yl)-acetamide, 200 µg Iodogen (1,3,4,6-tetrachloro-3α,6α-diphenyl-glycouril) and 74 MBq (2 mCi) [^125^I]NaI was added. The mixture was incubated for 90 min at room temperature. N,N-Diethyl-2-(2-(4-hydroxy-[^125^I]iodophenyl)-5,7-dimethyl-pyrazolo(1,5-a)pyrimidin-3-yl)-acetamide was purified with high-performance liquid chromatography (HPLC) to provide a 47% radiochemical yield. N,N-diethyl-2-(2-(4-hydroxy-[^125^I]iodophenyl)-5,7-dimethyl-pyrazolo(1,5-a)pyrimidin-3-yl)-acetamide was O-methylated with CH_3_I in the presence of K_2_CO_3_ to form [^125^I]iodoDPA-713 with a radiochemical yield of 86%. The [^125^I]iodoDPA-713 exhibited a radiochemical purity (as determined with HPLC) of >99% with a specific activity of 51.8 GBq/µmol (1.4 Ci/µmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iodoDPA-713%20and%20in%20vitro)]

In vitro autoradiography images of [^125^I]iodoDPA-713 binding/localization (or "affinity for") to PBR were obtained in frozen brain sections from normal and neurotoxicant-injected rats (9). Neurotoxicant induces inflammation in the brain. There was an increase in radioactivity in the cerebral cortex and hippocampus in the neurotoxicant-treated rat brains compared with the control brains. PK11195 (0.01 mM) completely blocked the increase of radioactivity in the neurotoxicant-treated rat brain.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iodoDPA-713%20and%20rodentia)]

Wang et al. (9) reported a preliminary SPECT/CT study in mice treated with lipopolysaccharide to induce inflammation in the lungs. Radioactivity was 1.5-fold higher in the inflamed lungs than in the normal lungs at 1 h after injection of [^125^I]iodoDPA-713. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iodoDPA-713%20and%20%28dog%20or%20sheep%20or%20pig%20or%20rabbit%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iodoDPA-713%20and%20%28primate%20not%20human%29)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iodoDPA-713%20and%20human)]

No publications are currently available.

## NIH Support

CA92871, ES07062

## References

1 Mohler H., Okada T. (1977). Benzodiazepine receptor: demonstration in the central nervous system. Science.
2 Hunkeler W., Mohler H., Pieri L., Polc P., Bonetti E.P., Cumin R., Schaffner R., Haefely W. (1981). Selective antagonists of benzodiazepines. Nature.
3 Olsen R.W., Tobin A.J. (1990). Molecular biology of GABAA receptors. Faseb J.
4 Anholt R.R., Pedersen P.L., De Souza E.B., Snyder S.H. (1986). The peripheral-type benzodiazepine receptor. Localization to the mitochondrial outer membrane. J Biol Chem.
5 Jones H.A., Valind S.O., Clark I.C., Bolden G.E., Krausz T., Schofield J.B., Boobis A.R., Haslett C. (2002). Kinetics of lung macrophages monitored in vivo following particulate challenge in rabbits. Toxicol Appl Pharmacol.
6 Kuhlmann A.C., Guilarte T.R. (2000). Cellular and subcellular localization of peripheral benzodiazepine receptors after trimethyltin neurotoxicity. J Neurochem.
7 Zavala F., Lenfant M. (1987). Benzodiazepines and PK 11195 exert immunomodulating activities by binding on a specific receptor on macrophages. Ann N Y Acad Sci.
8 James M.L., Fulton R.R., Henderson D.J., Eberl S., Meikle S.R., Thomson S., Allan R.D., Dolle F., Fulham M.J., Kassiou M. (2005). Synthesis and in vivo evaluation of a novel peripheral benzodiazepine receptor PET radioligand. Bioorg Med Chem.
9 Wang H., Pullambhatla M., Guilarte T.R., Mease R.C., Pomper M.G. (2009). Synthesis of [(125)I]iodoDPA-713: a new probe for imaging inflammation. Biochem Biophys Res Commun.